# (R)-2,3,4,5,6,7-Hexahydro-1-[4-[1-[4-(2-[^11^C]methoxyphenyl)piperazinyl]]-2-phenylbutyryl]-1H-azepine

Chemical name: | (R)-2,3,4,5,6,7-Hexahydro-1-[4-[1-[4-(2-[^11^C]methoxyphenyl)piperazinyl]]-2-phenylbutyryl]-1H-azepine
Abbreviated name: | (R)-[^11^C]RWAY, [^11^C]RWAY
Synonym:
Agent category: | Compound
Target: | 5-HT_1A_ serotonin receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[P ubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RWAY)]

Serotonin (5-hydroxytryptamine, 5-HT) has diverse physiologic roles as a neurotransmitter in the central nervous system (1). 5-HT is involved in regulation and modulation of sleep, affective and personality behaviors, and pain. It also is a regulator of smooth muscle function and platelet aggregation. The brain cortical 5-HT system has been implicated in several neuropsychiatric disorders, including major depression, anxiety, schizophrenia, and obsessive-compulsive disorder (2, 3). The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), many of which include several subtypes (4). There are five receptor subtypes within the G protein–coupled 5-HT_1_ receptor family: 5-HT_1A_, 5-HT_1B_, 5-HT_1D_, 5-HT_1E_, and 5-HT_1F_.

5-HT_1A_ receptors are abundantly present in the hippocampus, entorhinal cortex, frontal cortex, raphe nucleus, and septum, and the lowest densities are observed in the basal ganglia, substantia nigra, and cerebellum (5). Some thalamic and hypothalamic nuclei have intermediate densities. 5-HT_1A_ receptors are involved in the mediation of emotion and the function of the hypothalamus. 5-HT_1A_ receptors are implicated in anxiety, depression, hallucinogenic behavior, motion sickness, and eating disorders (6). Thus, there is a need for selective ligands to investigate the pharmacologic role of 5-HT_1A_ receptors.

There have been several studies to develop specific 5-HT_1A_ radioligands [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-HT1a%5BAll%20Fields%5D%20AND%20imaging%5BAll%20Fields%5D)] for positron emission tomography (PET) imaging, such as [carbonyl-^11^C]WAY 100635 (http://www.ncbi.nlm.nih.gov/books/NBK23263/), [^18^F]FPWAY (http://www.ncbi.nlm.nih.gov/books/NBK23137/), and [^18^F]MPPF (http://www.ncbi.nlm.nih.gov/books/NBK23391/). However, some of these compounds lack resistance to in vivo metabolism (7), which may cause difficulties in using the reference region method for determination of 5-HT_1A_ receptor densities in the brain. (R)-2,3,4,5,6,7-Hexahydro-1-[4-[1-[4-(2-methoxyphenyl)piperazinyl]]-2-phenylbutyryl]-1H-azepine (RWAY) is structurally similar to WAY100635 with the direction of its amide group reversed, which might be less susceptible to amide hydrolysis in vivo. RWAY was reported to be a potent antagonist of 5-HT_1A_ receptors (K_i_ = 0.6 nM) (8). This led to the development of (R)-2,3,4,5,6,7-Hexahydro-1-[4-[1-[4-(2-[^11^C]methoxyphenyl)piperazinyl]]-2-phenylbutyryl]-1H-azepine ([^11^C]RWAY) as a useful tool for in vivo PET imaging of the 5-HT_1A_ receptor. However, a relatively slow washout of radioactivity from the human brain likely reflects the accumulation of radiometabolite(s) in human brain (9). Therefore, the use of [^11^C]RWAY has been discontinued in humans.

### Related Resource Links:

- Chapters in MICAD (5-HT_1A_ (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=5-HT1A+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (5-HT_1A_ (http://www.ncbi.nlm.nih.gov/gene/3350))
- Articles in Online Mendelian Inheritance in Man (OMIM) (5-HT_1A_ (http://www.ncbi.nlm.nih.gov/omim/109760))
- Clinical trials (5-HT_1A_ (http://www.clinicaltrials.gov/ct2/results?term=5-HT1A))
- Drug information in Food and Drug Administration (5-HT_1A_ (http://google2.fda.gov/search?q=5-HT1a&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RWAY%20and%20synthesis)]

The radiosynthesis of [^11^C]RWAY reported by McCarron et al. (8) involved standard ^11^C-methylation of the corresponding desmethyl precursor (R)-2,3,4,5,6,7-hexahydro-1{4-[1[4-(2-hydroxyphenyl)-piperazinyl]]-2-phenylbutyryl}-1H-azepine with [^11^C]CH_3_I in DMF in the presence of tetrabutylammonium hydroxide at room temperature for 5 min. The reported overall radiochemical yield of the radiosynthesis from [^11^C]CO_2_ production was 33% at the end of synthesis (EOS), the specific radioactivity was 118 TBq/mmol (3,180 Ci/mmol), and the radiochemical purity was >99%. The total synthesis time was 35 min at EOS.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RWAY%20and%20in%20vitro)]

In vitro competition binding studies in cloned human 5-HT_1A_ receptors. (R)-RWAY had a binding affinity value (K_i_) of 0.60-1.88 nM (8). The Ki values were 7.2 nM for 5-HT2B, 9.5 nM for 5-HT1D and >65 nM for the remaining 5-HT subtypes. The affinity of RWAY for various biogenic amines, brain receptors, and transporters was determined to be 9-16 times lower than that of (R)-RWAY. There was a measurable free fraction of [^11^C]RWAY (2.9 ± 0.8%) in monkey plasma after 5 min incubation and 20 min centrifugation at room temperature.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RWAY%20and%20rodentia)]

Using small animal positron emission tomography (PET), Liow et al. (10) investigated rodent brain uptake of [^11^C]RWAY in control and cyclosporine A (CsA)-treated rats as well as P-glycoprotein (P-gp) knockout and wild type mice. [^11^C]RWAY and its radiometabolite in plasma and brain samples were determined at 30 min after injection. Regional brain binding potential (BP) values were calculated with a reference tissue (cerebellum) model. P-gp knockout mice had 2.5- and 2.8-fold greater brain accumulation of [^11^C]RWAY than wild type ones as measured by in vivo PET and ex vivo tissue sampling, respectively. Similarly, CsA increased rat brain accumulation 4.9- and 5.3-fold, in vivo PET and ex vivo. In addition, CsA increased the plasma free fraction of [^11^C]RWAY in rats by 2.7-fold. Although CsA increased brain accumulation in wild type mice by 2.5-fold, it had no effect on plasma free fraction in knockout animals. Three radiometabolites [^11^C]RWAY were uniformly distributed in rat brain, suggesting they were inactive. CsA treatment increased brain accumulation of [^11^C]RWAY and only one of its radiometabolites. Regional rat brain BP increased 27-70% in the CsA-treated rats and the P-gp knockout mice. [^11^C]RWAY is a P-gp substrate in rat and mouse. The effects of CsA in rats are mediated by both P-gp blockade and displacement of the radiotracer from plasma proteins.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RWAY%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RWAY%20and%20nonhuman%20primate)]

PET imaging was studied by McCarron et al. (8) in the brain of rhesus monkeys after intravenous injection of 196-218 MBq (5.29-5.90 mCi) of [^11^C]RWAY. Various brain regions exhibited rapid accumulation in 5-18 min with gradual decreases thereafter. [^11^C]RWAY PET images (up to 120 min after injection) displayed radioactivity concentrations that followed a rank order (tissue/cerebellum ratio): cingulate gyrus (6.4), frontal cortex (4.1), temporal cortex (3.8), raphe nucleus (2.1), and cerebellum (1.0) at 87.5 min. Pretreatment with WAY-100635 (antagonist, 0.5 mg/kg) 15 min prior to the injection of [^11^C]RWAY markedly reduced the radioactivity in the regions of interest to homogeneity at 15 min after tracer injection. Injection of WAY-100635 at 40 min after injection of [^11^C]RWAY immediately decreased the radioactivity levels in 5-HT1A receptor-rich regions. After injection of [^11^C]RWAY, 81.0 ± 4.3% and 14.0 ± 1.5% of the total plasma radioactivity was intact at 5 and 60 min, respectively. Three more hydrophilic metabolites were detected. Yasuno et al. (11) used mathematical modeling to show that the estimated values of regional BP were correlated strongly (r = 0.93-0.97) between two-tissue compartment model and multilinear reference tissue model with cerebellum as a reference region. The BP values of dorsal raphe nucleus, prefrontal cortex, and medial temporal region were 0.77-0.87, 1.45-1.57, and 1.68-1.79, respectively.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RWAY%20and%20human)]

Zhang et al. (9) studied [^11^C]RWAY PET in six healthy human subjects, using kinetic brain imaging and serial arterial measurements of plasma parent radiotracer. Brain receptor-rich regions/cerebellum ratios were ~3 at 80 min after injection. However, the washout from brain was unexpectedly slow relative to plasma clearance of the parent radiotracer. In both receptor-rich regions and cerebellum, distribution volumes were unstable and increased continuously from 90 to 150 min by about 30%. When the metabolites of [^11^C]RWAY in human and monkey were compared, a moderate lipophilic radiometabolite was present at a significantly higher percentage of total plasma radioactivity in humans (20.6%) than in monkeys (3.2%). The relatively slow washout of activity from brain and the temporal instability of distribution volume likely reflect the accumulation of radiometabolite(s) in human brain. Therefore, the use of [^11^C]RWAY has been discontinued in humans.

## Supplemental Information

[Disclaimers (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=disclaimer)]

Synthesis Protocol (http://www.ncbi.nlm.nih.gov/books/bookres.fcgi/micad/RWAYProtocol.pdf)

Toxicology (http://www.ncbi.nlm.nih.gov/books/bookres.fcgi/micad/RWAYTox.pdf)

Preclinical Pharmacology (http://www.ncbi.nlm.nih.gov/books/bookres.fcgi/micad/RWAYPharmPreC.pdf)

Animal Dosimetry (http://www.ncbi.nlm.nih.gov/books/bookres.fcgi/micad/RWAYADosim.doc)

## NIH Support

Intramural Research Program

## References

1 Lucki I. (1998). The spectrum of behaviors influenced by serotonin. Biol Psychiatry.
2 Fletcher A., Cliffe I.A., Dourish C.T. (1993). Silent 5-HT1A receptor antagonists: utility as research tools and therapeutic agents. Trends Pharmacol Sci.
3 Hoyer D., Clarke D.E., Fozard J.R., Hartig P.R., Martin G.R., Mylecharane E.J., Saxena P.R., Humphrey P.P. (1994). International Union of Pharmacology classification of receptors for 5-hydroxytryptamine (Serotonin). Pharmacol Rev.
4 Lanfumey L., Hamon M. (2004). 5-HT1 receptors. Curr Drug Targets CNS Neurol Disord.
5 Pazos A., Probst A., Palacios J.M. (1987). Serotonin receptors in the human brain--III. Autoradiographic mapping of serotonin-1 receptors. Neuroscience.
6 Cowen P.J. (2000). Psychopharmacology of 5-HT(1A) receptors. Nucl Med Biol.
7 Slifstein M., Parsey R.V., Laruelle M. (2000). Derivation of [(11)C]WAY-100635 binding parameters with reference tissue models: effect of violations of model assumptions. Nucl Med Biol.
8 McCarron, J.A., S.S. Zoghbi, H.U. Shetty, E.S. Vermeulen, H.V. Wikstrom, M. Ichise, F. Yasuno, C. Halldin, R.B. Innis, and V.W. Pike, Synthesis and initial evaluation of [(11)C](R)-RWAY in monkey-a new, simply labeled antagonist radioligand for imaging brain 5-HT(1A) receptors with PET. Eur J Nucl Med Mol Imaging, 2007
9 Zhang X.Y., Yasuno F., Zoghbi S.S., Liow J.S., Hong J., McCarron J.A., Pike V.W., Innis R.B. (2007). Quantification of serotonin 5-HT1A receptors in humans with [11C](R)-(-)-RWAY: radiometabolite(s) likely confound brain measurements. Synapse.
10 Liow J.S., Lu S., McCarron J.A., Hong J., Musachio J.L., Pike V.W., Innis R.B., Zoghbi S.S. (2007). Effect of a P-glycoprotein inhibitor, Cyclosporin A, on the disposition in rodent brain and blood of the 5-HT1A receptor radioligand, [11C](R)-(-)-RWAY. Synapse.
11 Yasuno F., Zoghbi S.S., McCarron J.A., Hong J., Ichise M., Brown A.K., Gladding R.L., Bacher J.D., Pike V.W., Innis R.B. (2006). Quantification of serotonin 5-HT1A receptors in monkey brain with [11C](R)-(-)-RWAY. Synapse.